# ^68^Ga-Isothiocyanatobenzyl-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine

Chemical name: | ^68^Ga-Isothiocyanatobenzyl-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine
Abbreviated name: | ^68^Ga-SCN-Bz-DOTA-NI, ^68^Ga-5
Synonym:
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Hypoxia
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole)]

Hypoxia is found in a variety of solid tumors and leads to tumor progression and resistance to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized, polarographic, oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7).

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging in 1979 (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic conditions, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). In normoxic conditions, the reduced molecule is rapidly reoxidized and transported from the cell. [^18^F]Fluoromisonidazole ([^18^F]FMISO (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FMISO)) is the most widely used positron emission tomography (10) tracer for imaging tumor hypoxia (7). However, it has slow clearance kinetics and a high lipophilicity, resulting in substantial background in PET scans. [^18^F]Fluoroazomycinarabinofuranoside ([^18^F]FAZA (http://www.ncbi.nlm.nih.gov/books/NBK23282/)) is a 2-nitroimidazole with a sugar addition (11) and has been studied as a hypoxia-imaging agent, showing promising results in various tumor models in rats and mice (12, 13). ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine (^68^Ga-DOTA-NI, ^68^Ga-4) and ^68^Ga-isothiocyanatobenzyl-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine (^68^Ga-SCN-Bz-DOTA-NI, ^68^Ga-5) were prepared for hypoxic tissue imaging (14).

### Related Resource Links:

- Chapters in MICAD (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Hypoxia-inducible factor 1, alpha subunit (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3091))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hypoxia (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hypoxia%5BAll+Fields%5D))
- Clinical trials (Hypoxia imaging (http://www.clinicaltrials.gov/ct2/results?term=hypoxia+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20synthesis)]

Hoigebazar et al. (14) synthesized two nitroimidazole derivatives by conjugating nitroimidazole and DOTA via an amide bond and a thiourea bond. A solution mixture of 2-(2-nitroimidazolyl)ethylamine (0.08 mmol) and DOTA (0.12 mmol) was incubated overnight at room temperature to yield DOTA-2-(2-nitroimidazolyl)ethylamine employing an amide bond linkage (DOTA-NI, 4). DOTA-NI was purified with high-performance liquid chromatography. To label with ^68^Ga, a mixture of DOTA-NI and ^68^GaCl_3_ was heated in acetate buffer (pH 3) for 10 min at 100°C. ^68^Ga-DOTA-NI was purified with cartridge filtration. Labeling yields were >98%. ^68^Ga-SCN-Bz-DOTA-NI was prepared similarly using a thiourea bond linkage with labeling yields of >98%. Both agents were stable at room temperature for 2 h with low protein binding. ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI are hydrophilic and have low partition coefficients (log P) of −4.6 and −4.5, respectively. The specific activities of ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI were 4.81 GBq/nmol (0.13 Ci/nmol) and 7.77 GBq/nmol (0.21 Ci/nmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20in%20vitro)]

In vitro studies indicated that uptake values of both ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI in cells from the Hela human cell line and the CT-26 mouse colon cell line were significantly higher (n = 4, P < 0.05) under hypoxic conditions for 4 h than under normoxic conditions after 60 min of incubation (2.4 times in Hela cells, 6.8 times in CT-26 cells for ^68^Ga-DOTA-NI; 2.1 times in Hela cells, 3.4 times in CT-26 cells for ^68^Ga-SCN-Bz-DOTA-NI) (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20rodentia)]

Ex vivo biodistribution studies of ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI in mice (n = 4/group) bearing CT-26 tumors exhibited rapid clearance of the tracer from the body over time (10, 30, 60, and 120 min after injection) (14). The highest uptake values were found in the kidneys, with ~10% injected dose/gram (ID/g) for ^68^Ga-DOTA-NI and ~15% ID/g for ^68^Ga-SCN-Bz-DOTA-NI at 10 min after injection. The liver and intestine accumulation values of ^68^Ga-SCN-Bz-DOTA-NI at 60 min (~3% ID/g, respectively) were higher than those of ^68^Ga-DOTA-NI (~1% ID/g, respectively) at the same time point. The initial tumor uptake values for ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI at 10 min after injection were 3.17% ID/g and 2.78% ID/g , respectively. These radioactivity levels declined over time for both tracers. The tumor/muscle ratios for ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI, which were ~0.65, at 60 min after injection were lower than those for [^18^F]FAZA (3.27) and [^18^F]FMISO (1.19) at the same time point, whereas the tumor/muscle ratios for ^68^Ga-DOTA-NI (~3.5) and ^68^Ga-SCN-Bz-DOTA-NI (~3.5) at 60 min after injection were higher than those for [^18^F]FAZA (1.7) and [^18^F]FMISO (1.7) at the same time point (15).

Tumor standardized uptake values (SUVs) at 30 min and 60 min after injection for ^68^Ga-DOTA-NI (0.81 ± 0.10 and 0.53 ± 0.10, respectively) and ^68^Ga-SCN-Bz-DOTA-NI (0.31 ± 0.10 and 0.17 ± 0.10, respectively) were determined with PET imaging in mice bearing CT-26 tumors (14). The tumor SUV/muscle SUV ratios of ^68^Ga-DOTA-NI were 5.08 ± 2.2 and 5.64 ± 0.8 at 30 min and 60 min, respectively. The tumor SUV/muscle SUV ratios of ^68^Ga-SCN-Bz-DOTA-NI were 1.86 ± 0.3 and 3.83 ± 0.8 at 30 min and 60 min, respectively. Both tracers showed high accumulation in the kidneys and urinary bladder.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20humans)]

No publication is currently available.

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Pulkkanen K.J., Laukkanen J.M., Fuxe J., Kettunen M.I., Rehn M., Kannasto J.M., Parkkinen J.J., Kauppinen R.A., Pettersson R.F., Yla-Herttuala S. (2002). The combination of HSV-tk and endostatin gene therapy eradicates orthotopic human renal cell carcinomas in nude mice. Cancer Gene Ther.
11 Reischl G., Ehrlichmann W., Bieg C., Solbach C., Kumar P., Wiebe L.I., Machulla H.J. (2005). Preparation of the hypoxia imaging PET tracer [18F]FAZA: reaction parameters and automation. Appl Radiat Isot.
12 Piert M., Machulla H.J., Picchio M., Reischl G., Ziegler S., Kumar P., Wester H.J., Beck R., McEwan A.J., Wiebe L.I., Schwaiger M. (2005). Hypoxia-specific tumor imaging with 18F-fluoroazomycin arabinoside. J Nucl Med.
13 Sorger D., Patt M., Kumar P., Wiebe L.I., Barthel H., Seese A., Dannenberg C., Tannapfel A., Kluge R., Sabri O. (2003). [18F]Fluoroazomycinarabinofuranoside (18FAZA) and [18F]Fluoromisonidazole (18FMISO): a comparative study of their selective uptake in hypoxic cells and PET imaging in experimental rat tumors. Nucl Med Biol.
14 Hoigebazar L., Jeong J.M., Hong M.K., Kim Y.J., Lee J.Y., Shetty D., Lee Y.S., Lee D.S., Chung J.K., Lee M.C. (2011). Synthesis of 68Ga-labeled DOTA-nitroimidazole derivatives and their feasibilities as hypoxia imaging PET tracers. Bioorg Med Chem.
15 Hoigebazar L., Jeong J.M., Choi S.Y., Choi J.Y., Shetty D., Lee Y.S., Lee D.S., Chung J.K., Lee M.C., Chung Y.K. (2010). Synthesis and characterization of nitroimidazole derivatives for 68Ga-labeling and testing in tumor xenografted mice. J Med Chem.